# Mono-[^123^I]Iodohypericin

Chemical name: | Mono-[^123^I]Iodohypericin
Abbreviated name: | [^123^I]MIH
Synonym:
Agent Category: | Compound
Target: | Necrotic tissue
Target Category: | Uptake
Method of detection: | Single-photon emission computed tomography (SPECT) or gamma planar imaging
Source of signal: | ^123^I
Activation: | No
Studies: | - Rodents; - Non-primate non-rodent mammals | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+iodohypericin&WebEnv=0LSJXItbyZpfOoLAxRkJw7yKUCzMQHmgkliOoh9-mz__oNJCvB_4UxFySy70V_g1QHwmv5bzpQLNwJP%407748428072881B60_0000SID&WebEnvRq=1)]

Approximately 2% of patients suffering from acute myocardial infarction (AMI) may be typically misdiagnosed on the basis of the presence of a characteristic chest pain or an altered electrocardiogram or biomarker pattern. Although this is only a small percentage of the total number of patients, the number of misdiagnosed AMI incidents is in the thousands because the total number of individuals suffering from AMI is very large (more than one million in the United States alone) (1). A quick diagnosis of AMI is important to devise a suitable treatment and increase the chances of a favorable outcome. The use of scintigraphic agents such as pyrophosphate labeled with radioactive technetium (^99m^Tc), which targets the calcium phosphate deposit in the myocardial tissue, or the F(ab) fragment of an anti-myosin antibody (labeled with radioactive indium), or [^99m^Tc]glucarate has been attempted for the diagnosis of AMI, but all these agents have some limitations (2). The pyrophosphate shows a low affinity and specificity for the necrotic myocardium in AMI patients, and the antibody is no longer available commercially (2). Although [^99m^Tc]glucarate appears to be a promising agent for the detection and quantification of infarct AMI, it is rapidly washed out from the infarcted myocardium; thus, a meaningful scan can be obtained only for a short time (<9 h) after the infarct has occurred because in the necrotic tissue it targets positively charged histones, which disintegrate rapidly (2). Myocardial perfusion imaging is also performed with other radiopharmaceuticals using either positron-emission tomography (PET) or single-photon emission computed tomography (SPECT), but all these agents have limitations as described in detail by Cuocolo et al. (3).

Hypericin, a polycyclic polyaromatic quinone found in the Saint John's wort plant (Hypericum perforatum), was shown to possess antiviral and antineoplastic characteristics (4). This compound has a chemical structure that is similar to some porphyrin derivatives that were shown to be photosensitizers that specifically targeted the necrotic tissue in neoplastic tumors and could be used for photodynamic therapy of cancer (5). Because porphyrins bound primarily to the necrotic tissue, they were also used by investigators as magnetic resonance imaging contrast agents to visualize AMI under preclinical conditions (6, 7). Bearing this in mind, investigators have evaluated the use of hypericin for the detection and imaging of necrotic tissue, including that which results from AMI (8-11). To achieve this, hypericin was derivatized with radioactive iodine (^123^I) to obtain mono-[^123^I]iodohypericin ([^123^I]MIH) and then used for SPECT imaging studies (8-11).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+hypericin+synthesis&WebEnv=0R_L7WKfSqOn2Vjs9D1Nx1ir_1cjdHDoB2zzEYJqTpGEwrkk3lzh8QWi8PdZC8LYvg2Kvh5jJ1wcab%407748428072881B60_0000SID&WebEnvRq=1)]

The synthesis of hypericin from emodin was patented and described elsewhere by Mazur et al. (12).

Hypericin was radioiodinated using an electrophilic substitution reaction with sodium [^123^I]iodide ([^123^I]Na) (11). Briefly, hypericin in ethanol, phosphoric acid, and peracetic acid were successively added to [^123^I]Na in sodium hydroxide. The mixture was incubated for 30 min at room temperature, and the reaction products were purified with reverse-phase high-performance liquid chromatography on a reverse-phase C_18_ column. The fractions containing [^123^I]MIH were concentrated under a flow of nitrogen at 45°C. The reaction yield was reported to be 70 to 97% relative to the starting ^123^I activity. The specific activity of [^123^I]MIH was reported to be >25 Ci/μmol (>925 GBq/μmol) with a purity of >99% up to 24 h after formulation. The final formulation was not described in this publication (11). However, in other publications [^123^I]MIH was reported to be formulated in 20% polyethylene glycol-400 immediately before administration (8, 9).

In one study, the biological activities of [^123^I]MIH and it precursor, mono-[^123^I]iodoprotohypericin ([^123^I]MIprotoH) were compared (see below in Rodent section under Animal Studies) (9). The synthesis of [^123^I]MIprotoH was described by Fonge et al. (9).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+hypericin+in+vitro&WebEnv=0-M68yPtCrO-l47QF9LFNJHh6kmcZSnJmj6sPl65Qpt1nPQfpkrHbrkpOtZbWm1ecYYoUnd-k5w%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+hypericin+rodentia&WebEnv=0FGwSSIaiS2No7Q3zfoaI6WbBNghLHVXXWAVoOqxEBjb00UG_0FAU3oIYxT47LsnJU4Syb2imAh%407748428072881B60_0000SID&WebEnvRq=1)]

A preliminary biodistribution study of [^123^I]MIH was performed by Vanbilloen et al. in mice bearing a radiation-induced fibrosarcoma tumor (13). The clearance of [^123^I]MIH from the blood was reported to be slow and primarily via the hepatobiliary route. Although the uptake of [^123^I]MIH was initially high in the lungs, it decreased gradually from 32.5% of the injected dose/g tissue (% ID/g) at 10 min to 16.2% ID/g at 24 h. During the same time period there was a gradual increase of [^123^I]MIH accumulation in the tumor, which reached a peak of 21.3% ID/g. From these results the investigators concluded that [^123^I]MIH was probably accumulating in the tumors because it bound to the necrosed part of the tumor. This observation prompted them to evaluate the use of this radiochemical for the detection of necrotic tissue in other organs of the body.

In another study, NMRI mice were injected with [^123^I]MIH and killed at various time points ranging from 10 min to 24 h (n = 3 animals per time point) after administration of the radiochemical (11). The various organs and body parts were collected, and the accumulated radioactivity was counted. Approximately 30% of the injected dose was still present in the blood at 4 h after injection, probably because hypericin is lipophilic and binds to both high- and low-density lipoproteins in plasma (14). The investigators observed that 70% ID was excreted with the feces after 24 h, and <10% ID was excreted in the urine; almost no uptake was observed in the brain (11). The investigators also noted that imaging with [^123^I]MIH was possible only 12 h after administration because they had to allow the blood concentration of the radiochemical to drop to a suitable level for imaging.

Ni et al. evaluated the use of [^123^I]MIH for the detection of necrosis in the rat liver (8). Images were obtained from normal (control) rats and rats with reperfused hepatic infarction 24 and 48 h after [^123^I]MIH injection. The accumulation of radioactivity was observed only in the necrotic part of reperfused hepatic infarction animal livers that had 3.1% ID/g versus 0.38% ID/g in the normal liver lobes. Presence of necrosis in the liver lobes showing a high accumulation of [^123^I]MIH was confirmed with histochemical staining (8).

The tumor-seeking properties of [^123^I]MIH and [^123^I]MIprotoH, a precursor of [^123^I]MIH, were compared using a radiation-induced fibrosarcoma mouse model (9). Both radiochemicals were reported to clear rapidly from all organs and accumulated to a similar extent (P > 0.05) in the tumors. The clearance of [^123^I]MIH from the blood and liver was faster than [^123^I]MIprotoH. In addition, the tumor/blood, tumor/liver, and tumor/spleen+pancreas ratios were higher for [^123^I]MIH than for [^123^I]MIprotoH 24 h after administration (5.4, 1.5, and 1.7, respectively, versus 0.4, 0.1, and 0.1, respectively). This indicated that, compared to its precursor molecule, [^123^I]MIH was a superior tracer for imaging tumors (9).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+hypericin+non+primate+mammals&WebEnv=04Nqf0KDpIuoZ2hqDqgcqxiKW3HrUNGT3pCN-kwFsgYX-G_NgLCtOUp_GV3-m7xInbxk1jBAKA-%407748428072881B60_0000SID&WebEnvRq=1)]

The use of [^123^I]MIH for imaging necrotic tissue in the myocardium as a result of AMI was investigated in a rabbit model (8, 10). A single New Zealand rabbit with occlusive myocardial infarction was injected with [^123^I]MIH and imaged 24 and 48 h after injection (8). Whole-body SPECT consistently showed a single spot in the anatomical area of the heart at both time points. The SPECT images also detected low levels of radioactivity in the thyroid and the intestines of the injected animals. Ex vivo histochemical staining and autoradiography of the myocardium confirmed that the radioactivity observed in the heart was indeed only in the infarcted regions.

In another study, Fonge et al. evaluated the use of [^123^I]MIH for the detection and quantification of AMI in a rabbit model and compared it with the use of radioactive [^13^N]ammonia ([^13^N]NH_3_) for the same purpose (10). Rabbits with an occluded left circumflex coronary artery (LCx) were divided into four groups. In group A (n = 3 animals), the artery was permanently occluded; in groups B (n = 3) and C (n = 6), the artery was reperfused by releasing the occlusion after 15 and 90 min, respectively; group D (n = 2) served as the control group in that the artery was not occluded at all. The animals were imaged with PET using [^13^N]NH_3_ 18 h after induction of the infarct followed by an injection of [^123^I]MIH for SPECT imaging at different time points. The animals were then killed, and the excised hearts were sliced for autoradiography and histochemical staining. In the control animals (group D), [^13^N]NH_3_ was evenly distributed throughout the left ventricular wall, but the other animals with LCx (groups A, B, and C) showed left-ventricular perfusion defects to different degrees depending on the infarct size. The infarcts were clearly visible with SPECT imaging only 9 h after and for up to 24 h after the injection of [^123^I]MIH. The investigators reported a perfect match between the PET and SPECT images. Autoradiography revealed that only the rabbits in group C had a strong uptake of [^123^I]MIH, and animals in groups A, B, and D showed a low uptake of the radiochemical. Also, on histological examination only rabbits in groups A, B, and C showed myocardial injury that correlated with the degree of necrosis induced by occlusion of the LCx.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+iodohypericin+non+human+primates&WebEnv=0i6tboeBAHDIbase8APELCnxfv0scyZk__WEQzgY3VATtqgGEHUH9qANUMIuh-0tTQB3bh8dIAd%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+iodohypericin+humans&WebEnv=0ek1VLxxlFV7IjHiHL7L8TiPE9ot4fT5XqAWk1qWiILXjNjqavhiTDMBky2I_CNePPgtgIWhz5M%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## References

1 Pope J.H., Aufderheide T.P., Ruthazer R., Woolard R.H., Feldman J.A., Beshansky J.R., Griffith J.L., Selker H.P. (2000). Missed diagnoses of acute cardiac ischemia in the emergency department. N Engl J Med.
2 Flotats A., Carrio I. (2003). Non-invasive in vivo imaging of myocardial apoptosis and necrosis. Eur J Nucl Med Mol Imaging.
3 Cuocolo A., Acampa W., Imbriaco M., De Luca N., Iovino G.L., Salvatore M. (2005). The many ways to myocardial perfusion imaging. Q J Nucl Med Mol Imaging.
4 Miskovsky P. (2002). Hypericin--a new antiviral and antitumor photosensitizer: mechanism of action and interaction with biological macromolecules. Curr Drug Targets.
5 Magro C.M., Abbas A.E., Ross P. (2006). The application of photodynamic therapy in the treatment of metastatic endobronchial disease. Lasers Surg Med.
6 Lee S.S., Goo H.W., Park S.B., Lim C.H., Gong G., Seo J.B., Lim T.H. (2003). MR imaging of reperfused myocardial infarction: comparison of necrosis-specific and intravascular contrast agents in a cat model. Radiology.
7 Choi S.I., Choi S.H., Kim S.T., Lim K.H., Lim C.H., Gong G.Y., Kim H.Y., Weinmann H.J., Lim T.H. (2000). Irreversibly damaged myocardium at MR imaging with a necrotic tissue-specific contrast agent in a cat model. Radiology.
8 Ni Y., Huyghe D., Verbeke K., de Witte P.A., Nuyts J., Mortelmans L., Chen F., Marchal G., Verbruggen A.M., Bormans G.M. (2006). First preclinical evaluation of mono-[123I]iodohypericin as a necrosis-avid tracer agent. Eur J Nucl Med Mol Imaging.
9 Fonge H., Van de Putte M., Huyghe D., Bormans G., Ni Y., de Witte P., Verbruggen A. (2007). Evaluation of tumor affinity of mono-[(123)I]iodohypericin and mono-[(123)I]iodoprotohypericin in a mouse model with a RIF-1 tumor. Contrast Media Mol Imaging.
10 Fonge H., Vunckx K., Wang H., Feng Y., Mortelmans L., Nuyts J., Bormans G., Verbruggen A., Ni Y. (2008). Non-invasive detection and quantification of acute myocardial infarction in rabbits using mono-[123I]iodohypericin {micro}SPECT. Eur Heart J.
11 Bormans G., Huyghe D., Christiaen A., Verbeke K., de Groot T., Vanbilloen H., de Witte P., Verbruggen A. (2004). Preparation, analysis and biodistribution in mice of iodine-123 laballed derivatives of hypericin. J Label Comp Radiopharm.
12 Mazur, Y., H. Bock, and D. Lavie, Preparation of hypericin., in United States Patent Office, U.S.P. Office, Editor. 1992, Yeda Research and Development Co. Ltd.: United States.
13 Vanbilloen H., Bormans G., Chen B., de Witte P., Verbruggen A., Verbeke K. (2001). Synthesis and preliminary evaluation of mono-[123I]iodohypericin. J Label Comp Radiopharm.
14 Lavie G., Mazur Y., Lavie D., Meruelo D. (1995). The chemical and biological properties of hypericin--a compound with a broad spectrum of biological activities. Med Res Rev.